# ^125^I-Labeled heparin-binding peptides that target heparan sulfate proteoglycans for the in vivo imaging of peripheral amyloidosis

Chemical name: | ^125^I-Labeled heparin-binding peptides that target heparan sulfate proteoglycans for the in vivo imaging of peripheral amyloidosis
Abbreviated name: | [^125^I]-Peptides
Synonym:
Agent Category: | Peptides
Target: | Heparan sulfate proteoglycans
Target Category: | Proteins (proteoglycans)
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planer imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Peripheral%20amyloidosis&cmd=DetailsSearch)]

Peripheral amyloidosis (http://www.nlm.nih.gov/medlineplus/amyloidosis.html) is the extracellular deposition of insoluble protein fibrils in various organs of animals, including humans, and these deposits are considered to be biomarkers for diseases such as Alzheimer’s disease (AD), light chain amyloidosis (AL), etc (1). The fibrils are made up of disease-specific aggregated proteins or peptides (e.g., Aβ peptides for AD, light chains for AL or multiple myeloma, and reactive amyloidosis (AA)) that incorporate heparin sulfate proteoglycans (HSPG; heparin belongs to the heparan sulfate family of proteoglycans that contain the (GlcNS6S-IdoA2S)_3_ motif) and the serum amyloid P component (SAP) within their structure during disease progression. A characteristic feature of the protein fibrils is that the constituent proteins form a secondary cross-β pleated sheet structure that is resistant to proteolytic digestion (for structural details, see Goldsbury et al. (2)). The HSPG contain diverse types of oligosaccharides that are sulfated on the hydroxyl moieties to varying degrees, and these hypersulfated structures are distinct, are found specifically in the amyloid deposits, and differ from one another depending on the organ where they are located (3). In addition, clinical symptoms in patients are influenced by the degree to which an organ is involved in the disease (4). Because the HSPG are hypersulfated compared to proteoglycans found in normal tissues, HSPG are considered to be relevant biomarkers for use with noninvasive imaging to detect, diagnose, and monitor amyloidosis progression and to determine the prognosis for a patient with amyloidosis (1).

Whole-body scintigraphy with radioiodinated SAP is commonly used in Europe for the detection of amyloidosis in the various parts of the body, but this technique is not approved for clinical use in the United States by the U.S. Food and Drug Administration because the SAP in the tracer is isolated from human sources (1). In an attempt to develop an amyloid imaging agent that does not require the use of materials of human origin, Wall et al. studied the biodistribution of seven ^125^I-labeled synthetic heparin-binding peptides with small-animal single-photon emission computed tomography (SPECT) to evaluate their use in the detection of amyloid deposits in mice with severe systemic AA amyloidosis (1).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Amyloid+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/search/open/condition=%22Amyloidosis%22) related to amyloidosis

Amyloidosis in Online Mendelian Inheritance in Man Database (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=amyloidosis)

Protein (http://www.ncbi.nlm.nih.gov/protein/AAA35526.1) sequence of human amyloid

Crystal structures (http://www.ncbi.nlm.nih.gov/structure?term=Human%20amyloid%20proteins) of human amyloid proteins

Symptoms, diagnosis, and treatment of amyloidosis (http://www.cedars-sinai.edu/Patients/Health-Conditions/Amyloidosis.aspx?gclid=CJbMzuybm6wCFYTe4AodsyAo1g) (at Cedars-Sinai Medical Center, LA)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-peptide%20synthesis&cmd=DetailsSearch)]

The ^125^I-labeled heparin-binding peptides (designated p1 thru p7; see table below for amino acid sequences) were obtained in a semi-pure form from commercial sources and purified with reversed-phase liquid chromatography using a C_3_ reversed-phase column as described by Wall et al. (1). The mass of each purified peptide was confirmed with mass spectroscopy. The amino acid sequences of the various peptides used in the study are given below:

Peptide | Amino acid sequence | Net charge
p1 | CGGYS SSRPV RRRRR PRVSR RRRRG GRRRR | +16
p2 | CGGYG DAKKK KDGKK AEPKN PRENK LKQPG | +6
p3 | CGGYP KKGSK KAVTK AQKKD GKKR | +9
p4 | CGGYS RPRAR ARARD QTR | +5
p5 | CGGYS KAQKA QAKQA KQAQK AQKAQ AKQAK Q | +8
p6 | CGGYP RRRRS SSRPI RRRRP RRASRR | +13
p7 | CGGYF AKLNC RLYRK ANKSS K | +6

Each peptide was labeled with ^125^I using the chloramine-T method, and the purity of the labeled product was determined with SDS/PAGE followed by analysis with a phosphor imager. The radiochemical yield and purity of the ^125^I-labeled peptides were not reported. The specific activity of the labeled peptides was calculated to be ~0.75 MBq/μg (~20 μCi/μg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-peptide%20in%20vitro%20studies&cmd=DetailsSearch)]

The heparin-binding characteristics of the various purified peptides were investigated with high-salt elution of the peptide from a heparin column (1). The heparin-binding activity of the peptides was reported to be p1 > p6 > p4 > p5 = p3 > p7 > p2 and was dependent on the net charge (see table in Synthesis).

Using histochemical techniques (exposure of tissue sections to biotinylated p% peptide followed by detection with streptavidin-conjugated horse radish peroxidase), the p5 peptide was shown to bind the Aβ amyloid deposits in the brain sections of patients with AD (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-labeled%20heparin%20binding%20peptides%20studies%20in%20rodentia&cmd=DetailsSearch)]

Wall et al. investigated the biodistribution of the various ^125^I-labeled peptides in H2-L^d^-huIL-6 Tg BALB/c transgenic mice (AA mice; constitutively express the human IL-6 transgene) 3–6 weeks after the induction of AA amyloidosis in the animals (1). The animals (n = 3 mice/radioiodinated peptide/time point) were injected with 3.70–7.40 MBq (100–200 μCi; 5–10 μg protein) of each ^125^I-peptide through the tail vein. For use as controls, the labeled peptides were administered to the same number of wild-type (WT) mice as described above. The mice were subsequently euthanized at 1 h and 4 h postinjection (p.i.) to determine the amount of radioactivity accumulated in the major organs. Data obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). At 1 h p.i., the amount of radioactivity accumulated in the liver with peptides p1, p2, p3, p4, p5, p6 and p7 was 11.6 ± 3.4% ID/g, 3.1 ± 1.0% ID/g, 6.0 ± 1.4% ID/g, 5.8 ± 0.7% ID/g, 12.5 ± 2.5% ID/g, 6.6 ± 1.5% ID/g, and 4.1 ± 0.1% ID/g, respectively; in the pancreas, accumulation was 7.1± 2.1% ID/g, 3.5 ± 1.4% ID/g, 5.6 ± 2.3% ID/g, 6.3 ± 1.9% ID/g, 10.0 ± 4.5% ID/g, 4.8 ± 0.3% ID/g, and 3.7 ± 0.5% ID/g, respectively; in the spleen, accumulation was 11.5 ± 2.2% ID/g, 2.4 ± 0.4% ID/g, 3.0 ± 1.7% ID/g, 5.6 ± 0.4% ID/g%, 15.9 ± 5.2% ID/g, 6.3 ± 0.4% ID/g, and 2.8 ± 0.6% ID/g, respectively. Presence of AA amyloid in the various tissues was confirmed with Congo Red staining (this stain is selective for amyloid deposits). From the biodistribution study it was evident that the amount of radioactivity in the organs of mice with AA amyloidosis was at least two- to seven-fold higher than radioactivity in organs of the WT animals. Among all the peptides, the uptake of radioactivity in the liver, spleen, and pancreas was highest with ^125^I-labeled p5. The AA amyloidosis/WT uptake (AA/WT) ratios for the liver and spleen were ~5 and 8, respectively, which increased to ~10 and >20, respectively, at 4 h p.i. On the basis of these observations, the efficacy of the peptides to bind the amyloid deposits was determined to be p5 > p1 > p6 > p4 ~ p3 > p7 > p2. These observations were confirmed with microradioautography of the liver and spleen tissues.

SPECT/ computed tomography imaging of the AA and WT mice at 1 h p.i. showed that the amyloid deposits could be visualized in the liver, pancreas, spleen, and kidneys of AA animals only with p1, p5, and, to some extent, p6 (1). At 4 h p.i., the liver and spleen were visible only in AA animals injected with the p1 or p5 peptides. In comparison, regardless of the radioiodinated peptide injected, SPECT images of the WT mice acquired at 1 h p.i. showed that the label was present only in the thyroid and the stomach of the animals.

In another study, the amyloid binding of radioiodinated p1 and p5 (because with these peptides the different organs showed the highest uptake compared to the other peptides) was studied in mice (n = 3 animals/time point) up to 24 h p.i (1). Except for the liver, pancreas, and spleen, all amyloid-free organs in the mice showed rapid loss of radioactivity during this period. In addition, the retention of radiolabeled p5 was higher than that from labeled p1 in all organs with amyloid deposits. The whole-body clearance T_1/2eff_ values of ^125^I-labeled p1 and p5 for the WT mice were calculated to be 1.2 ± 0.01 h and 1.1 ± 0.1 h, respectively. The T_1/2eff_ values of the radioiodinated peptides in the AA mice were 3.3 ± 0.08 h and 2.3 ± 0.3 h, respectively. SPECT images of the mice acquired at 24 h p.i. showed that the liver and spleen were visible only in animals injected with p5. These organs were not visible after 8 h p.i. in the animals injected with the labeled p1 peptide. The precise location of amyloid deposits observed in the liver and spleen of AA animals injected with the labeled p5 peptide was confirmed with autoradiography and by the co-localization Congo Red stain in the tissue sections of these organs.

From these studies, the investigators concluded that the p5 peptide is a potential noninvasive imaging agent for the detection and monitoring of amyloidosis in patients (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-labeled%20heparin%20binding%20peptides%20studies%20in%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-labeled%20heparin%20binding%20peptides%20studies%20in%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-labeled%20heparin%20binding%20peptides%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies reported in this chapter were supported by National Institute of Diabetes and Digestive and Kidney Diseases Award R01DK079984.

## References

1 Wall J.S., Richey T., Stuckey A., Donnell R., Macy S., Martin E.B., Williams A., Higuchi K., Kennel S.J. (2011). In vivo molecular imaging of peripheral amyloidosis using heparin-binding peptides. Proc Natl Acad Sci U S A.
2 Goldsbury C., Baxa U., Simon M.N., Steven A.C., Engel A., Wall J.S., Aebi U., Muller S.A. (2011). Amyloid structure and assembly: insights from scanning transmission electron microscopy. J Struct Biol.
3 Ori A., Wilkinson M.C., Fernig D.G. (2008). The heparanome and regulation of cell function: structures, functions and challenges. Front Biosci.
4 Perfetto F., Moggi-Pignone A., Livi R., Tempestini A., Bergesio F., Matucci-Cerinic M. (2010). Systemic amyloidosis: a challenge for the rheumatologist. Nat Rev Rheumatol.